# Microbubbles conjugated with anti-vascular cell adhesion molecule-1 nanobody cAbVCAM1-5

Chemical name: | Microbubbles conjugated with anti-vascular cell adhesion molecule-1 nanobody cAbVCAM1-5
Abbreviated name: | MB-cAbVCAM1-5, µB-cAbVCAM1-5
Synonym:
Agent category: | Antibody
Target: | Vascular cell adhesion molecule-1 (VCAM-1)
Target category: | Adhesion molecule
Method of detection: | Ultrasound (US)
Source of signal: | Microbubbles
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VCAM-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VCAM-1+microbubble)]

Ultrasound is a widely used imaging modality (1), and its role in noninvasive molecular imaging with ligand-carrying microbubbles (MBs) is expanding (2). MBs are comprised of spherical cavities encapsulated in a shell and filled with a gas. The shells are made of phospholipids, surfactants, denatured human serum albumin, or synthetic polymers. Ligands and antibodies can be incorporated into the MB shell surface. MBs are usually 2–8 μm in size. MBs of this size provide a strongly reflective interface and resonate to ultrasound waves. They are used as ultrasound contrast agents in imaging of inflammation, angiogenesis, intravascular thrombus, and tumors (2-4). They also can potentially be used for drug and gene delivery (5).

Endothelial cells are important cells in inflammatory responses (6, 7). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their ability to adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (8).

VCAM-1 is found in very low amounts or non-detectable on the cell surface of resting endothelial cells and other vascular cells, such as smooth muscle cells and fibroblasts (9-13). VCAM-1 binds to very late antigen-4 (VLA-4) integrin on the cell surface of leukocytes. IL-1 and TNFα increase expression of VCAM-1 and other cell adhesion molecules on the vascular endothelial cells, which leads to leukocyte adhesion to the activated endothelium. Furthermore, VCAM-1 expression was also induced by oxidized low-density lipoproteins under atherogenic conditions (14). Overexpression of VCAM-1 by atherosclerotic lesions plays an important role in their progression toward vulnerable plaques, which may erode and rupture. MBs targeted with monoclonal antibody against VCAM-1 are being developed as a noninvasive agent for VCAM-1 expression in vascular endothelial cells during different stages of inflammation in atherosclerosis (15). Nanobodies are the smallest intact antigen-binding fragments (15 kDa) isolated from heavy-chain camelid antibodies with efficient and specific tumor targeting (16-18). Hernot et al. (19) prepared an anti-VCAM-1 nanobody (cAbVCAM1-5) that was site-specifically biotinylated in bacteria. cAbVCAM1-5 was coupled to biotinylated lipid MBs via streptavidin-biotin bridging to form MB-cAbVCAM1-5 for use with in vivo ultrasound imaging of VCAM-1 expression.

### Related Resource Links:

- Chapters in MICAD (VCAM-1 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=VCAM-1+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (VCAM-1 (http://www.ncbi.nlm.nih.gov/gene/7412))
- Articles in Online Mendelian Inheritance in Man (OMIM) (VCAM-1 (http://www.ncbi.nlm.nih.gov/omim/192225))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+attachment)]

For targeted MBs, Hernot et al. (19) prepared biotinylated MBs by sonication of an aqueous dispersion of decafluorobutane gas, phosphatidylcholine, polyoxyethylene-40-stearate, and phosphatidylethanolamine-polyethylene glycol(PEG3400)-biotin. MBs were combined with streptavidin, washed, and conjugated with 62.5 pmol/10^7^ MBs biotinylated nanobody cAbVCAM1-5 against VCAM-1 (MBcAbVCAM1-5) or control nanobody against eGFP (MBcAbGFP4). The targeted MBs were about 2.2 ± 0.2 μm in diameter with a polydispersity index of 1.32. An antibody to MB ratio was estimated with flow cytometry to be 288,000 ± 38,000. There were ~10,000 nanobodies per μm^2^ of the MB surface.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+in+vitro)]

Binding experiments with biotinylated cAbVCAM1-5 were performed with the use of a Biacore sensor chip immobilized with mouse VCAM-1 protein (20). The K_d_ value of biotinylated cAbVCAM1-5 was calculated to be 7.2 nM as compared with 10.7 nM for the non-biotinylated nanobody.

Hernot et al. (19) performed perfusion of MBcAbVCAM1-5 (2.5 × 10^6^/ml) through the flow chamber coated with endothelial cells at a wall shear rate of 1.0–5.0 dynes/cm^2^. There was a significantly greater number of MBcAbVCAM1-5 attached to TNF^_^activated mouse endothelial cells than to normal endothelial cells at 1.0 dynes/cm^2^ (P < 0.01). The attachment of MBcAbVCAM1-5 to activated endothelial cells decreased with increasing shear rates, with still significant MB adhesion at 5.0 dynes/cm^2^ (P < 0.05). The adhesion of MBcAbVCAM1-5 to the activated endothelial cells was inhibited by 70% with excess non-biotinylated cABVCAM1-5 (P < 0.01). No attachment of control MBcAbGFP4 to normal and activated endothelial cells was observed. Flow cytometry showed binding of cAbVCAM1-5 to activated mouse endothelial cells but not to non-activated cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+rodentia)]

Hernot et al. (19) determined MBcAbVCAM1-5 attachment to the tumor vasculatures in mice (n = 4) bearing MC38 subcutaneous tumors. Contrast-enhanced ultrasound molecular imaging of the tumors was performed for ~12 minutes after intravenous injection of 3.75 × 10^7^ MBcAbVCAM1-5 or MBcAbGFP4. Contrast-enhanced signals peaked at 20 s after injection of MBs. The tumor signal of MBcAbVCAM1-5 declined more slowly than that of MBcAbGFP4. The tumor signal (expressed as % of maximal intensity at 20 s) of MBcAbVCAM1-5 (44 ± 9%) was 100% higher than that of MBcAbGFP4 (22 ± 10%) (P < 0.05) at 10 min after injection. After destruction of the MBs with two high-intensity ultrasound pulses at 10 min, the signals completely disappeared, indicating that the majority of unbound circulating MBs had cleared from the blood. Immunohistochemical analysis of the tumor sections showed expression of VCAM-1 in the tumor vasculature as well as on the tumor cells. No blocking studies were performed with cAbVCAM1-5.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Microbubbles+VCAM-1+and+human)]

No publication is currently available.

## NIH support

R21/33 CA102880

## References

1 Wells P.N. (2001). Physics and engineering: milestones in medicine. Med Eng Phys.
2 Lindner J.R. (2004). Microbubbles in medical imaging: current applications and future directions. Nat Rev Drug Discov.
3 Klibanov A.L. (2005). Ligand-carrying gas-filled microbubbles: ultrasound contrast agents for targeted molecular imaging. Bioconjug Chem.
4 Villanueva F.S., Wagner W.R., Vannan M.A., Narula J. (2004). Targeted ultrasound imaging using microbubbles. Cardiol Clin.
5 Dijkmans P.A., Juffermans L.J., Musters R.J., van Wamel A., ten Cate F.J., van Gilst W., Visser C.A., de Jong N., Kamp O. (2004). Microbubbles and ultrasound: from diagnosis to therapy. Eur J Echocardiogr.
6 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
7 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
8 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
9 Bochner B.S., Luscinskas F.W., Gimbrone M.A., Newman W., Sterbinsky S.A., Derse-Anthony C.P., Klunk D., Schleimer R.P. (1991). Adhesion of human basophils, eosinophils, and neutrophils to interleukin 1-activated human vascular endothelial cells: contributions of endothelial cell adhesion molecules. J Exp Med.
10 Kume N., Cybulsky M.I., Gimbrone M.A. (1992). Lysophosphatidylcholine, a component of atherogenic lipoproteins, induces mononuclear leukocyte adhesion molecules in cultured human and rabbit arterial endothelial cells. J Clin Invest.
11 Leung K.H. (1999). Release of soluble ICAM-1 from human lung fibroblasts, aortic smooth muscle cells, dermal microvascular endothelial cells, bronchial epithelial cells, and keratinocytes. Biochem Biophys Res Commun.
12 Luscinskas F.W., Cybulsky M.I., Kiely J.M., Peckins C.S., Davis V.M., Gimbrone M.A. (1991). Cytokine-activated human endothelial monolayers support enhanced neutrophil transmigration via a mechanism involving both endothelial-leukocyte adhesion molecule-1 and intercellular adhesion molecule-1. J Immunol.
13 Nagel T., Resnick N., Atkinson W.J., Dewey C.F., Gimbrone M.A. (1994). Shear stress selectively upregulates intercellular adhesion molecule-1 expression in cultured human vascular endothelial cells. J Clin Invest.
14 Aikawa M., Libby P. (2004). The vulnerable atherosclerotic plaque: pathogenesis and therapeutic approach. Cardiovasc Pathol.
15 Kaufmann B.A., Sanders J.M., Davis C., Xie A., Aldred P., Sarembock I.J., Lindner J.R. (2007). Molecular imaging of inflammation in atherosclerosis with targeted ultrasound detection of vascular cell adhesion molecule-1. Circulation.
16 Arbabi Ghahroudi M., Desmyter A., Wyns L., Hamers R., Muyldermans S. (1997). Selection and identification of single domain antibody fragments from camel heavy-chain antibodies. FEBS Lett.
17 Desmyter A., Decanniere K., Muyldermans S., Wyns L. (2001). Antigen specificity and high affinity binding provided by one single loop of a camel single-domain antibody. J Biol Chem.
18 Muyldermans S. (2001). Single domain camel antibodies: current status. J Biotechnol.
19 Hernot S., Unnikrishnan S., Du Z., Shevchenko T., Cosyns B., Broisat A., Toczek J., Caveliers V., Muyldermans S., Lahoutte T., Klibanov A.L., Devoogdt N. (2012). Nanobody-coupled microbubbles as novel molecular tracer. J Control Release.
20 Broisat A., Hernot S., Toczek J., De Vos J., Riou L.M., Martin S., Ahmadi M., Thielens N., Wernery U., Caveliers V., Muyldermans S., Lahoutte T., Fagret D., Ghezzi C., Devoogdt N. (2012). Nanobodies Targeting Mouse/Human VCAM1 for the Nuclear Imaging of Atherosclerotic Lesions. Circ Res.